# [^18^F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine

Chemical name: | [^18^F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine | [image]
Abbreviated name: | [^18^F]6 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Sigma-1 (σ1) receptor | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]6

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma-1%20receptors%20and%20imaging)]

[^18^F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine, abbreviated as [^18^F]6, is a piperazine derivative synthesized by Moussa et al. for positron emission tomography (PET) of sigma-1 (σ1) receptor (1).

σ1 receptor is a protein that is widely distributed in both the central nervous system (CNS) and peripheral organs. There are at least two subtypes of σ receptors, σ1 and σ2 receptors. Although the functions of σ2 receptor are poorly understood, σ1 receptor is believed to act as a modulator of the signal transduction in neurotransmitter systems (2, 3). σ1 receptor primarily resides at the interface between the endoplasmic reticulum and mitochondria, where it modulates Ca^2+^ flux by acting as a molecular chaperone for type 3 inositol-1,4,5-triphosphate receptors. σ1 receptor can also translocate to the plasma membrane, where it regulates the voltage-dependent Ca^2+^ channels, K^+^ channels, and other membrane-bound proteins (1, 2).

More and more evidence suggests that σ1 receptor is involved in a range of CNS diseases such as affective disorders, psychosis, schizophrenia, substance abuse, Parkinson’s disease, and Alzheimer’s disease (1, 4). Studies on postmortem human brains have shown that the density of σ1 receptor decreased in patients with schizophrenia and Alzheimer’s disease (5). Discovery of specific ligands for σ1 receptor has further prompted investigations in the imaging and treatment of neuropsychiatric diseases by targeting σ1 receptor (3, 4).

Noninvasive imaging of σ1 receptor in vivo would enable better understanding of the pathogenesis of neuropsychiatric diseases as well as how the expression and function of σ1 receptors change during disease progression (2). Early in 1998, Baziard-Mouysset et al. synthesized a series of disubstituted 1,4-piperazines, flanked by a chromene ring and a benzyl group (6). Of this series, the simplest compound that contained an unsubstituted benzyl ring displayed high affinity for σ receptors (K_i_ = 3 nM) and negligible off-target activity. Substitution of the benzyl ring was generally detrimental to σ binding, with the exception of 4-chloro or 4-methoxy substitution, which marginally improved σ receptor binding (K_i_ = 1 nM and 0.6 nM, respectively). The chromene ring was shown to have little effect on σ binding, and it was well tolerated for substitution with a large number of alternate aromatic groups (7). With the 2-benzofurylmethyl group–substituted compound as a lead compound, Moussa et al. generated a series of N-(2-benzofuranylmethyl)-N'-(alkoxybenzyl)piperazines as selective σ1 receptor ligands (1, 4, 8). Two compounds in this series, N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine (compound 6) and N-(benzofuran-2-ylmethyl)-N'-(4'-methoxybenzyl)piperazine (compound 13), were further radiolabeled and tested for their feasibilities as imaging probes for σ1 receptors.

This chapter summarizes the data obtained with [^18^F]6.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=sigma-1%20receptors) and protein (http://www.ncbi.nlm.nih.gov/protein?term=sigma-1%20receptors) sequences of sigma-1 (σ1) receptors

Sigma-1 (σ1) receptor-related compounds (http://www.ncbi.nlm.nih.gov/pcsubstance?term=sigma-1%20receptors) in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21962578)]

Moussa et al. described the synthesis of piperazine derivatives in detail (1, 4). Compound 6 was synthesized by O-alkylation of N-(2-benzofuranylmethyl)-N'-(4-hydroxybenzyl)piperazine (compound 7) with 2-fluoroethyl tosylate. The synthesis of [^18^F]6 was achieved in two steps from compound 7. Mono-alkylation of compound 7 with 1,2-ethylene glycol bis-tosylate furnished tosylated precursor compound 8. Compound 8 was then radiofluorinated with a Tracerlab FXF-N module. The overall synthesis time for [^18^F]6 was 45 min, and the radiochemical yield was 18%. Both radiochemical and chemical purities were >98%, with a specific activity of 45 GBq/μmol (1.22 Ci/µmol) at end of synthesis. [^18^F]6 was formulated by dilution of the radioactive fraction of the high-performance liquid chromatography (HPLC) mobile phase with water for injection. The final preparation was free from precursor 8. Administration to the animal was performed within 30 min after the end of synthesis.

The lipophilicity of compound 6 was evaluated with HPLC, which gave a log D value of 3.35 (1). To ensure high uptake in the brain and to minimize non-specific binding, the optimal log D value for therapeutic CNS-active compounds is reported to be between 2 and 3.5.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21962578)]

Affinities of compound 6 for σ1 and σ2 receptors were determined with competitive displacement of [^3^H](+)-pentazocine in a rat brain homogenate preparation (to determine σ1 receptor affinity) and with competitive displacement of [^3^H]1,3-di-(2-tolyl)-guanidine in a PC12 cell preparation (a rat pheochromocytoma cell line known to overexpress σ2 receptors) (1, 4). Compound 6 had K_i_ values of 2.6 nM and 486 nM for σ1 and σ2 receptors, respectively, indicating selectivity for σ1 over σ2. The K_i_ values of compound 6 for 5-HT_1A_, 5-HT_2B_, and D_2_ receptors were 2,439, 96, and >10,000 nM, respectively (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21962578)]

MicroPET studies were conducted in an anaesthetized Papio hamadryas baboon to evaluate the in vivo regional distribution kinetics of [^18^F]6 after intravenous administration of 100 MBq (2.7 mCi) [^18^F]6 (1). The microPET images confirmed the ability of [^18^F]6 to penetrate the blood–brain barrier with accumulation in the baboon brain. The time-activity curve showed that [^18^F]6 reached the maximal level within 5 min after injection and remained at a plateau to the end of the PET scan (60 min after injection). Homogenous uptake of [^18^F]6 was observed in the cortex, striatum, thalamus, and cerebellum, which are known to express σ receptors.

The in vivo specificity of [^18^F]6 uptake was evaluated in a single blocking study in the same baboon (1). Pretreatment with haloperidol (1 mg/kg) 5 min before [^18^F]6 administration resulted in increased radioligand uptake within 3 min, followed by a rapid decline to the washout level within 5 min after injection. The net result was an 80% reduction in radioligand uptake in all regions of the brain at the end of the imaging experiment (60 min.) when compared to [^18^F]6 administration alone, indicating the in vivo specificity of [^18^F]6 for σ receptors. Haloperidol is a high-affinity ligand for σ receptors.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=21417461)]

No references are currently available.

## References

1 Moussa I.A., et al. (2011). Synthesis and in vivo evaluation of [18F]N-(2-benzofuranylmethyl)-N'-[4-(2-fluoroethoxy)benzyl]piperazine, a novel sigma1 receptor PET imaging agent. Bioorg Med Chem Lett.
2 Diaz J.L., et al. (2009). Selective sigma-1 (sigma1) receptor antagonists: emerging target for the treatment of neuropathic pain. Cent Nerv Syst Agents Med Chem.
3 Berardi F., et al. (2009). 1-Cyclohexylpiperazine and 3,3-dimethylpiperidine derivatives as sigma-1 (sigma1) and sigma-2 (sigma2) receptor ligands: a review. Cent Nerv Syst Agents Med Chem.
4 Moussa I.A., et al. (2010). Design, synthesis, and structure-affinity relationships of regioisomeric N-benzyl alkyl ether piperazine derivatives as sigma-1 receptor ligands. J Med Chem.
5 Jansen K.L., et al. (1993). Loss of sigma binding sites in the CA1 area of the anterior hippocampus in Alzheimer's disease correlates with CA1 pyramidal cell loss. Brain Res.
6 Baziard-Mouysset G., et al. (1998). Synthesis and structure-activity relationships of novel 2-amino alkyl chromones and related derivatives as s site-selective ligands. Eur J Med Chem.
7 Younes S., et al. (2000). Synthesis and structure-activity relationships of novel arylalkyl 4-benzyl piperazine derivatives as sigma site selective ligands. Eur J Med Chem.
8 Moussa I.A., et al. (2011). Effects of linker elongation in a series of N-(2-benzofuranylmethyl)-N'-(methoxyphenylalkyl)piperazine sigma(1) receptor ligands. Bioorg Med Chem Lett.